# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid- cyclic arginine-glycine-aspartic acid peptide

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-cyclic arginine-glycine-aspartic acid peptide
Abbreviated name: | ^64^Cu-DOTA-c(RGDyK)
Synonym: | ^64^Cu-c(RGDyK)
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^64^Cu
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29)]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid -cyclic arginine-glycine-aspartic acid peptide [^64^Cu-DOTA-c(RGDyK)] is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature, tumor angiogenesis, and osteoclasts (1).

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). Chen et al. (1) evaluated a cyclic RGD peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumor. They used DOTA for c(RGDyK) conjugation with ^64^Cu. ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20synthesis)]

Chen et al. (1) reported the synthesis of ^64^Cu-DOTA-c(RGDyK). The cyclic peptide was first prepared via solution cyclization of fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by trifluoroacetic acid deprotection in the presence of the free radical scavenger triisopropylsilane. DOTA was obtained commercially. DOTA-c(RGDyk) conjugate was prepared with the use of 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) to activate DOTA at pH 5.5 for 30 min at 4ºC. The c(RGDyk) peptide in water at 4ºC was added to the reaction mixture, and the pH was adjusted to 8.5. The reaction was allowed to incubate overnight at 4ºC. The resultant DOTA-c(RGDyk) conjugate was purified by semi-preparative high-performance liquid chromatography (HPLC) with a yield of 79%. The purified product was labeled with ^64^Cu by addition of ^64^Cu in the ratio of 2–5 μg peptide per 37 MBq (1 mCi) ^64^Cu in 0.1 N sodium acetate (pH 5.5) buffer. This was followed by incubation at 50ºC for 45 minutes. ^64^Cu-DOTA-c(RGDyK) was purified with a C-18 Sep-Pak cartridge using 85% ethanol as the elution solvent. The radiochemical yield was ≥90%, and the radiochemical purity was ≥98%. The specific activity ranged from 7.4–18.5 GBq/μmol (200–500 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20rodentia)]

Biodistribution studies of ^64^Cu-DOTA-c(RGDyK) were conducted in mice bearing MDA-MB-435 human breast cancer (1). Each mouse received an i.v. dose of 370 kBq (10 μCi) ^64^Cu-DOTA-c(RGDyK). Rapid blood clearance of the radioactivity from the blood circulation was observed. The tumor radioactivity levels (n = 5) in percent injected dose per g (% ID/g) for the tumor were 2.02 ± 0.15 (0.25 h), 1.98 ± 0.10 (0.5 h), 1.90 ± 0.36 (1 h), 1.36 ± 0.10 (2 h), and 1.44 ± 0.09 (4 h). The tumor/blood ratios were 1.67 ± 0.11 (0.25 h), 3.72 ± 0.18 (0.5 h), 8.14 ± 0.88 (1 h), 6.94 ± 0.51 (2 h), and 6.00 ± 0.06 (4 h). The liver, kidneys, and intestine were the organs with similar or slightly higher radioactivity levels than the tumor. A co-injection dose of 10 mg/kg c(RGDyK) decreased the tumor radioactivity level to 0.34 ± 0.02% ID/g (n = 4) at 1 h. MicroPET imaging of tumor-bearing mice injected with 14.8 MBq (0.4 mCi) ^64^Cu-DOTA-c(RGDyK) visualized the tumor with clear contrast. The tumor/muscle ratio at 2 h was 5.6 ± 0.4 (n = 3). In comparison, the tumor/muscle ratios from the biodistribution and autoradiography studies were 6.0 ± 0.6 and 6.9 ± 0.8 (n = 3), respectively. Co-injection with different amounts of c(RGDyK) revealed a dose-dependent blocking effect on the tumor radioactivity level.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIBIB R21 EB001785, NCI P20 CA86532, R24 CA86307.

## References

1 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.